# ^86^Y-CHX-A''-Diethylenetriamine pentaacetic acid-bevacizumab

Chemical name: | ^86^Y-CHX-A''-Diethylenetriamine pentaacetic acid-bevacizumab
Abbreviated name: | ^86^Y-CHX-A''-DTPA-bevacizumab
Synonym: | ^86^Y-CHX-A''-DTPA-avastin
Agent category: | Antibody
Target: | Vascular endothelial growth factor-A (VEGF-A)
Target category: | Antigen
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^86^Y
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=71051581), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_001025368.1) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=7422) for more information about VEGF-A.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=86Y%20bevacizumab)]

The vascular endothelial growth factor (VEGF) family is composed of five VEGF glycoproteins (VEGF-A, VEGF-B, VEGF-C, VEGF-D, and VEGF-E) and consists of at least six isoforms of various numbers of amino acids (121, 145, 165, 183, 189, and 206 amino acids) produced through alternative splicing (1). VEGF-A is composed of VEGF_121_, VEGF_165_, and VEGF_189_ isoforms, which are secreted by most cell types and are active as homodimers linked by disulfide bonds. VEGF_121_ does not bind to heparin like other VEGF species do (2). VEGF is a potent angiogenic factor that induces proliferation, sprouting, migration, and tube formation of endothelial cells. There are three high-affinity tyrosine kinase VEGF receptors (VEGFR-1, Flt-1; VEGFR-2, KDR/Flt-1; and VEGFR-3, Flt-4) on endothelial cells. Several types of non-endothelial cells, such as hematopoietic stem cells, melanoma cells, monocytes, osteoblasts, and pancreatic β cells, also express VEGFRs (1).

VEGF is overexpressed in various tumor cells and tumor-associated endothelial cells (3). Inhibition of VEGFR function has been shown to inhibit pathological angiogenesis as well as tumor growth and metastasis (4, 5). Radiolabeled VEGF has been developed as a single-photon emission computed tomography tracer for imaging solid tumors and angiogenesis in humans (6-8). However, several studies have shown that cancer treatments (photodynamic therapy, radiotherapy, and chemotherapy) can lead to increased tumor VEGF expression and subsequently to more aggressive disease (9, 10). Therefore, it is important to measure VEGF levels in the tumors to design better anticancer treatment protocols. Bevacizumab is a humanized antibody against VEGF-A (11) that binds to all VEGF-A isoforms. Bevacizumab is approved for clinical use in metastatic colon carcinoma and non-small cell lung cancer (12). VEGFR-2 has been shown to mediate most of the VEGF-A activation in tumor endothelial cells (13, 14). Nayak et al. (15) prepared ^86^Y-CHX-A''-diethylenetriamine pentaacetic acid-bevacizumab (^86^Y-CHX-A''-DTPA-bevacizumab) for imaging VEGF expression in nude mice bearing SKOV-3 human ovarian tumor xenografts.

### Related Resource Links:

- Chapters in MICAD (VEGF (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=VEGF+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (VEGFR-2 (http://www.ncbi.nlm.nih.gov/gene/3791)).
- Articles in Online Mendelian Inheritance in Man (OMIM) (VEGF (http://www.ncbi.nlm.nih.gov/omim/192240))
- Clinical trials (Bevacizumab (http://www.clinicaltrials.gov/ct2/results?term=Bevacizumab))
- Drug information in FDA (Bevacizumab (http://google2.fda.gov/search?q=bevacizumab%29+&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=10&y=10))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=86Y%20bevacizumab+synthesis)]

Bifunctional CHX-A''-DTPA was used to conjugate bevacizumab to form CHX-A''-DTPA-bevacizumab (~150 kDa), which was purified with column chromatography (15). The DTPA/antibody ratio was determined to be 1.9. Next, ^86^Y solution (140–170 MBq (3.8–4.6 mCi)) was added to CHX-A''-DTPA-bevacizumab (0.33 nmol) in ammonium acetate buffer (pH 5–6). The reaction mixture was incubated for 30 min at room temperature, and ^86^Y-CHX-A''-DTPA-bevacizumab was purified with column chromatography. The yield of ^86^Y-CHX-A''-DTPA-bevacizumab was 60%–75% with a specific activity of >220 MBq/nmol (6.1 mCi/nmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=86Y%20bevacizumab+in+vitro)]

Binding of ^86^Y-CHX-A''-DTPA-bevacizumab under excess antigen (VEGF_165_) conditions indicated that the immunoreactivity was 58%–66% (15). The non-specific binding was <6% in the assay.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=86Y%20bevacizumab+rodentia)]

Nayak et al. (15) performed ex vivo biodistribution studies of 0.5 MBq (0.014 mCi) ^86^Y-CHX-A''-DTPA-bevacizumab (0.02 nmol) in nude mice (n = 4/group) bearing human SKOV-3 ovarian tumor (VEGF-A–positive) and MSTO-211H mesothelioma (VEGF-A–negative) xenografts. SKOV-3 tumor uptake values were 12% injected dose per gram (ID/g) at 0.5 d, 17% ID/g at 3 d, and 15% ID/g at 4 d. On the other hand, MSTO-211H tumor uptake values were 5% ID/g at 0.5 d, 6% ID/g at 3 d, and 6% ID/g at 4 d. The radioactivity level in the blood was 11% ID/g at 0.5 d, 7% ID/g at 3 d, and 6% at 4 d. The initial uptake in the liver was 14% ID/g at 0.5 d and decreased to 8% ID/g at 3 d. All other organs showed lower radioactivity levels than the SKOV-3 tumors at all these time points. Coinjection of bevacizumab (0.33 nmol) with ^86^Y-CHX-A''-DTPA-bevacizumab reduced the SKOV-3 tumor accumulation to 9% ID/g at 3 d after injection, whereas no inhibition was observed in the MSTO-211H tumors and non-tumor tissues.

Nayak et al. (15) studied the whole-body distribution of 2 MBq (0.056 mCi) ^86^Y-CHX-A''-DTPA-bevacizumab (0.02 nmol) with PET imaging in nude mice (n = 3) bearing human SKOV-3 ovarian tumor and MSTO-211H xenografts with static scans at various time points (1–3 d). The SKOV-3 tumors were clearly visualized at 1–3 d after injection, but the MSTO-211H tumors were not. The mean tumor residence times were similar (2.6–2.7 d). Co-injection of 0.33 nmol bevacizumab inhibited accumulation of radioactivity in the SKOV-3 tumors by 50% at 3 d after injection, whereas no inhibition was observed in the MSTO-211H tumors. There was a good correlation (r^2^ = 0.87) between the tracer accumulation measured with PET and tracer accumulation measured with ex vivo biodistribution studies.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=86Y%20bevacizumab+and+(dog+or+sheep+or+pig+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=86Y%20bevacizumab+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=86Y%20bevacizumab+human)]

No publication is currently available.

## NIH Support

Intramural Research Program

## References

1 Ferrara N. (2004). Vascular endothelial growth factor: basic science and clinical progress. Endocr Rev.
2 Cohen T., Gitay-Goren H., Sharon R., Shibuya M., Halaban R., Levi B.Z., Neufeld G. (1995). VEGF121, a vascular endothelial growth factor (VEGF) isoform lacking heparin binding ability, requires cell-surface heparan sulfates for efficient binding to the VEGF receptors of human melanoma cells. J Biol Chem.
3 Soria J.C., Fayette J., Armand J.P. (2004). Molecular targeting: targeting angiogenesis in solid tumors. Ann Oncol.
4 Ferrara N. (2004). Vascular endothelial growth factor as a target for anticancer therapy. Oncologist.
5 Hicklin D.J., Ellis L.M. (2005). Role of the vascular endothelial growth factor pathway in tumor growth and angiogenesis. J Clin Oncol.
6 Li S., Peck-Radosavljevic M., Koller E., Koller F., Kaserer K., Kreil A., Kapiotis S., Hamwi A., Weich H.A., Valent P., Angelberger P., Dudczak R., Virgolini I. (2001). Characterization of (123)I-vascular endothelial growth factor-binding sites expressed on human tumour cells: possible implication for tumour scintigraphy. Int J Cancer.
7 Li S., Peck-Radosavljevic M., Kienast O., Preitfellner J., Hamilton G., Kurtaran A., Pirich C., Angelberger P., Dudczak R. (2003). Imaging gastrointestinal tumours using vascular endothelial growth factor-165 (VEGF165) receptor scintigraphy. Ann Oncol.
8 Li S., Peck-Radosavljevic M., Kienast O., Preitfellner J., Havlik E., Schima W., Traub-Weidinger T., Graf S., Beheshti M., Schmid M., Angelberger P., Dudczak R. (2004). Iodine-123-vascular endothelial growth factor-165 (123I-VEGF165). Biodistribution, safety and radiation dosimetry in patients with pancreatic carcinoma. Q J Nucl Med Mol Imaging.
9 Gorski D.H., Beckett M.A., Jaskowiak N.T., Calvin D.P., Mauceri H.J., Salloum R.M., Seetharam S., Koons A., Hari D.M., Kufe D.W., Weichselbaum R.R. (1999). Blockage of the vascular endothelial growth factor stress response increases the antitumor effects of ionizing radiation. Cancer Res.
10 Solban N., Selbo P.K., Sinha A.K., Chang S.K., Hasan T. (2006). Mechanistic investigation and implications of photodynamic therapy induction of vascular endothelial growth factor in prostate cancer. Cancer Res.
11 Wang Y., Fei D., Vanderlaan M., Song A. (2004). Biological activity of bevacizumab, a humanized anti-VEGF antibody in vitro. Angiogenesis.
12 Ferrara N., Hillan K.J., Gerber H.P., Novotny W. (2004). Discovery and development of bevacizumab, an anti-VEGF antibody for treating cancer. Nat Rev Drug Discov.
13 Folkman J. (2002). Role of angiogenesis in tumor growth and metastasis. Semin Oncol.
14 Ferrara N., Gerber H.P., LeCouter J. (2003). The biology of VEGF and its receptors. Nat Med.
15 Nayak, T.K., K. Garmestani, K.E. Baidoo, D.E. Milenic, and M.W. Brechbiel, PET imaging of tumor angiogenesis in mice with VEGF-A targeted (86)Y-CHX-A''-DTPA-bevacizumab. Int J Cancer, 2010